# ^64^Cu-Z-E-(1,8-Diamino-3,6,10,13,16,19-hexaazabicyclo(6,6,6)eicosane)-aminohexanoyl-Asp-Gly-Glu-Ala

Chemical name: | ^64^Cu-Z-E-(1,8-Diamino-3,6,10,13,16,19-hexaazabicyclo(6,6,6)eicosane)-aminohexanoyl-Asp-Gly-Glu-Ala
Abbreviated name: | ^64^Cu-Z-E(diamsar)-Ahx-DGEA
Synonym:
Agent category: | Peptide
Target: | Integrin α_2_β_1_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAF77577.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_002203.3) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3673) for more information about integrin α_2_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Z-E(diamsar)-Ahx-DGEA)]

Integrins are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events (e.g., cell adhesion, migration, differentiation, proliferation, and apoptosis) involving cell–cell and cell–matrix interactions (1, 2). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. On the other hand, integrins affect tumor growth, tumor invasiveness, and metastasis (3, 4). The α_2_β_1_ integrin receptor binds mainly collagen type I, laminins, E-cadherin, and matrix metalloproteinase 1 (5). The α_2_β_1_ integrin is strongly expressed on tumor cells and has been implicated in tumor progression and metastasis (6, 7). In particular, prostate cancer cells and prostate cancer stem cells express high levels of α_2_β_1_ integrin (8, 9). A tetrapeptide sequence consisting of Asp-Gly-Glu-Ala (DGEA) has been identified as a recognition motif used by the type I collagen to bind to α_2_β_1_ integrin (10). DGEA was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in prostate tumor-bearing mice (11). Cy5.5-DGEA has been shown to have a high accumulation in α_2_β_1_-positive PC-3 human prostate tumor cells in nude mice. For positron emission tomography (PET) imaging of α_2_β_1_ integrin, ^64^Cu-Z-E-(1,8-diamino-3,6,10,13,16,19-hexaazabicyclo(6,6,6)eicosane)-aminohexanoyl-Asp-Gly-Glu-Ala (^64^Cu-Z-E(diamsar)-Ahx-DGEA) was prepared and evaluated in nude mice bearing human PC-3 prostate tumors (12).

### Related Resource Links:

- Chapters in MICAD (DGEA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=DGEA+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_2_ integrin (http://www.ncbi.nlm.nih.gov/gene/3673), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_2_ integrin (http://www.ncbi.nlm.nih.gov/omim/192974), β_1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Z-E(diamsar)-Ahx-DGEA+synthesis)]

Z-E-(diamsar)-Ahx-DGEA peptides were obtained using solid-phase synthesis (12). The diamsar group was added to carboxy group of glutamic acid of Z-E-Ahx-DGEA peptides. The measured mass of Z-E(diamsar)-Ahx-DGEA peptides confirmed the 1:1 addition. Z-E-(diamsar)-Ahx-DGEA was incubated with [^64^Cu]acetate in ammonium acetate buffer (pH 5.5) for 30 min at 23–37°C. ^64^Cu-Z-E-(diamsar)-Ahx-DGEA was purified with high-performance liquid chromatography. This procedure provided a radiolabeling yield of >90%, with a specific activity of 10.7 GBq/µmol (0.29 Ci/µmol) and a radiochemical purity of >98%. ^64^Cu-Z-E-(diamsar)-Ahx-DGEA was 98% intact for 48 h at 40°C in phosphate-buffered saline.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Z-E(diamsar)-Ahx-DGEA+and+in+vitro)]

Flow cytometry analysis showed that 99.7% of PC-3 cells, 51.4% of CWR-22 cells, and 15.6% of LNCaP cells were positive for the α_2_β_1_ receptors using 5-Carboxyfluorescin-DGEA (FAM-DGEA) (11). Binding of 1 µM FAM-DGEA to the three cell types was analyzed with fluorescence microscopy. PC-3 cells exhibited a higher fluorescence intensity signal than CWR-22 and LNCaP cells. The binding of FAM-DGEA to PC-3 cells was completely blocked with 20 µM DGEA. Cellular accumulation of ^64^Cu-Z-E-(diamsar)-Ahx-DGEA in PC-3 cells was low, with <0.4% incubation dose at 2 h after incubation (13). No blocking studies were carried out.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Z-E(diamsar)-Ahx-DGEA+rodentia)]

Huang et al. (12) performed PET imaging in nude mice (n = 3) bearing PC-3 tumors at 30 min after injection of 11.1 MBq (0.3 mCi) ^64^Cu-Z-E-(diamsar)-Ahx-DGEA. The tumors were clearly visualized. The tumor accumulation values were 2.08 ± 0.47% injected dose/gram (ID/g). The liver and kidney accumulation values were 1.25 ± 0.25% ID/g and 2.8 ± 0.2% ID/g, respectively. ^64^Cu-Z-E-(diamsar)-Ahx-DGEA exhibited tumor/kidney, tumor/liver, and tumor/muscle ratios of 0.8, 1.8, and 5.8, respectively. Co-injection of DGEA (10 mg/kg) inhibited the tumor, kidney, liver, and muscle accumulation of ^64^Cu-Z-E-(diamsar)-Ahx-DGEA by 60%, 30%, 50%, and 5%, respectively, at 30 min after injection (13).

In another PET study, Huang et al. (13) performed imaging in nude mice (n = 3/group) bearing PC-3 tumors at 30, 60, and 120 min after injection of 9.16 MBq (0.25 mCi) ^64^Cu-Z-E-(diamsar)-Ahx-DGEA. The tumor accumulation values were 2.28 ± 0.47% ID/g, 0.94 ± 0.53% ID/g, and 0.36 ± 0.55% ID/g at 30, 60, and 120 min after injection, respectively. There was a rapid washout from the tumors as well as from the kidney, liver, and muscle. Co-injection of DGEA (10 mg/kg) reduced the PC-3 tumor accumulation to 0.9 ± 0.31%ID/g at 30 min after injection. In the CWR-22 control tumor, the uptake was 0.3 ± 0.2%ID/g at 30 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Z-E(diamsar)-Ahx-DGEA+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Z-E(diamsar)-Ahx-DGEA+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Z-E(diamsar)-Ahx-DGEA+human)]

No publication is currently available.

## References

1 Hynes R.O. (2009). The extracellular matrix: not just pretty fibrils. Science.
2 Barczyk M., Carracedo S., Gullberg D. (2010). Integrins. Cell Tissue Res.
3 Makrilia N., Kollias A., Manolopoulos L., Syrigos K. (2009). Cell adhesion molecules: role and clinical significance in cancer. Cancer Invest.
4 Brooks S.A., Lomax-Browne H.J., Carter T.M., Kinch C.E., Hall D.M. (2010). Molecular interactions in cancer cell metastasis. Acta Histochem.
5 Heino J. (2000). The collagen receptor integrins have distinct ligand recognition and signaling functions. Matrix Biol.
6 Barbolina M.V., Moss N.M., Westfall S.D., Liu Y., Burkhalter R.J., Marga F., Forgacs G., Hudson L.G., Stack M.S. (2009). Microenvironmental regulation of ovarian cancer metastasis. Cancer Treat Res.
7 Kirkland S.C., Ying H. (2008). Alpha2beta1 integrin regulates lineage commitment in multipotent human colorectal cancer cells. J Biol Chem.
8 Hall C.L., Dai J., van Golen K.L., Keller E.T., Long M.W. (2006). Type I collagen receptor (alpha 2 beta 1) signaling promotes the growth of human prostate cancer cells within the bone. Cancer Res.
9 Kiefer J.A., Farach-Carson M.C. (2001). Type I collagen-mediated proliferation of PC3 prostate carcinoma cell line: implications for enhanced growth in the bone microenvironment. Matrix Biol.
10 Staatz W.D., Fok K.F., Zutter M.M., Adams S.P., Rodriguez B.A., Santoro S.A. (1991). Identification of a tetrapeptide recognition sequence for the alpha 2 beta 1 integrin in collagen. J Biol Chem.
11 Huang C.W., Li Z., Conti P.S. (2011). In Vivo Near-Infrared Fluorescence Imaging of Integrin alpha2beta1 in Prostate Cancer with Cell-Penetrating-Peptide-Conjugated DGEA Probe. J Nucl Med.
12 Huang C.W., Li Z., Cai H., Shahinian T., Conti P.S. (2011). Biological stability evaluation of the alpha2beta1 receptor imaging agents: diamsar and DOTA conjugated DGEA peptide. Bioconjug Chem.
13 Huang C.W., Li Z., Cai H., Chen K., Shahinian T., Conti P.S. (2011). Design, synthesis and validation of integrin alpha2beta1-targeted probe for microPET imaging of prostate cancer. Eur J Nucl Med Mol Imaging.